# CLIO-(H-2K^d^)-Lys-Tyr-Asp-Lys-Ala-Asp-Val-Phe-Leu

Chemical name: | CLIO-(H-2K^d^)-Lys-Tyr-Asp-Lys-Ala-Asp-Val-Phe-Leu
Abbreviated name: | CLIO-NPR-V7
Synonym: | MN-NRP-V7
Agent category: | Peptide, protein (nanoparticle)
Target: | H-2K^d^-restricted β cell-specific T cell receptor (8.3-TCR)
Target category: | receptor
Method of detection: | Magnetic resonance imaging (MRI)
Source of signal/contrast: | Iron oxides
Activation: | No
Studies: | - In vitro; - Rodents | No structure is Currently available in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(CLIO-NRP-V7))]

Type 1 diabetes (T1D) is an organ-specific autoimmune disease originating from the destruction of pancreatic β cells by autoreactive T cells (TCs) (1). In particular, islet-associated CD8^+^ TCs initiate β cell insult and trigger shedding of β cell autoantigens. This subset of CD8^+^ TCs is primarily restricted to the class I major histocompatibility complex (MHC) molecule H-2K^d^ (2), in which Vα17-Jα42 TC receptor α (TCR-α) chains are expressed for recognition of a unique β cell autoantigen (1), islet-specific glycose-6-phosphatase catalytic subunit-related protein (IGRP). After initiation, a series of immune responses occur, including loading autoantigens into antigen-presenting cells (the dendritic cells), activating autoreactive CD4^+^ TCs, and infiltrating TCs in pancreatic islets. T1D development consists of an insulitis phase and a diabetes phase, which are readily reproduced in a murine model called non-obese diabetic (NOD) mouse for human T1D (3, 4). In general, the progression from insulitis to diabetes in NOD mice is accompanied by alternatively repeated circulation of IGRP_206-214_–reactive CD8^+^ TC pool and avidity maturation of its islet-associated counterpart (5). Thus, IGRP has been used as a target for human diabetogenic response. NOD peptide (NRP-V7) (Lys-Tyr-Asp-Lys-Ala-Asp-Val-Phe-Leu (KYNKANVEL)) is a mimotope of IGRP that shares a 67% sequence homology with the endogenous IGRP_206-214_ epitope and has high avidity for H-2K^d^ molecule (5). A transgenic mouse (8.3-NOD) that specifically expresses H-2K^d^–restricted TCR (8.3-TCR) has been used for a variety of therapeutic studies (6), in which 8.3-TCR constitutes as much as 30% to 40% of islet-associated CD8^+^ TCs (2).

Cross-linked iron oxide-(H-2K^d^)-(CLIO-NPR-V7) is a NRP-V7 labeled paramagnetic iron oxide nanoparticle that is used to image 8.3-TCR by magnetic resonance imaging (MRI) (1, 5). This agent consists of three components: an iron oxide nanoparticle core for MRI contrast enhancement, two avidin molecules are covalently linked to the core surface, and eight biotinylated peptide/MHC complex (NRP-V7/H-2K^d^) monomers bind on the avidins for recognition of 8.3-TCR. The nanoparticle contains an icosahedral core of superparamagnetic crystalline Fe_3_O_4_ (magnetite) that is caged by epichlorohydrin cross-linked dextran and functionalized with amine groups (CLIO-NH_2_) (7). They have a high magnetic susceptibility to induce a significant magnetization inside a magnetic field. This creates microscopic field gradients that diphase nearby protons and causes a shortening of T_2_ relaxation times (8). Avidin is a tetrameric protein with a molecular mass of 68 KDa that is capable of strongly binding four biotins (association constant (K_a_) = 1.7 × 10^15^ M^-1^) (9). Because CLIO-NRP-V7 binds to the peripheral 8.3-TCR in the blood directly, it can be used to label islet-associated TCs for in vivo tracking through systemic administration (1, 5).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(CLIO-NRP-V7) +AND+synthesis%0D%0A)]Moore et al. described the synthesis of CLIO-NRP-V7 in detail (1). Initially, monocrystalline iron oxide (MION) was synthesized by neutralization of ferrous salts, ferric salts, and dextran with ammonium hydroxide, followed by ultrafiltration (10). The obtained MION (~2,064 iron atoms per nanoparticle) was cross-linked in strong base with epichlorohydrin and then reacted with ammonia to produce aminated iron oxide nanoparticle CLIO-NH_2._ Next, fluorescein isothiocyanate (FITC)-labeled avidin was converted to its oxidized form using sodium periodate (1). The oxidized avidin was incubated with CLIO-NH_2_ (pH 9.5) for 2.5 h to form Schiff base on the surface of CLIO, which was further reduced to a stable covalent bond by reacting with sodium cyanoborohydride for 3.5 h. The avidin molecule per CLIO nanoparticle ratio, which was ~2 avidin molecules per CLIO, was obtained by measuring the concentration of avidin and iron. The average number of biotin binding sites on avidin-CLIO was determined to be ~8 (4 for each avidin). NRP-V7 peptide was obtained with standard solid-phase methods using fluorenylmethoxycarbonyl chemistry in an automated peptide synthesizer (2). H-2K^d^ molecules were immunoaffinity-purified from 1.4 × 10^10^ interferon (IFN)-γ–treated NIT-1 pancreatic β cells by using monoclonal antibody SF1-1.1(2). NRP-V7 formed stable complexes with H-2K^d^ molecule in aqueous solution. NRP-V7/H-2K^d^ was biotinylated with an enzymatic process (11). Then, CLIO-avidin was coupled with biotinylated monomer NRP-V7/H-2K^d^ at a molar ratio of 4 mol biotin per mol avidin to yield CLIO-NPR-V7 (1). The mean hydrodynamic sizes of the nanoparticles as measured with laser light scattering were 29.5 nm for CLIO-NH_2_, 66.8 nm for CLIO-avidin, and 114.1 nm for CLIO-NRP-V7. CLIO-NRP-V7 was found to bind with high molecular weight biotinylated proteins such as albumin by measuring it spin-spin relaxation time (T_2_) at 0.47 T.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(CLIO-NRP-V7) +AND+%22in+vitro%22)]

Moore et al. examined the specificity of CLIO-NRP-V7 for NRP-V7–reactive CD8^+^ TCs in vitro with the use of flow cytometry (1). CD8^+^ TCs derived from 8.3-NOD mice or wild-type NOD mice were incubated with iodinated CLIO-NRP-V7 (50 μg Fe) for 1 hr, and then the TCs were analyzed with fluorescence-activated cell sorting (FACS) and quantified with γ-counting. The labeling efficiency of CLIO-NRP-V7 was found to be 92% in 8.3-NOD–derived CD8^+^ TCs versus 1.86% in wild-type NOD mice, demonstrating a high specificity of CLIO-NRP-V7 for NRP-V7–reactive CD8^+^ TCs. As found with fluorescence microscopy, CLIO-NRP-V7 was predominantly located inside the cell labeled by the internalization of TCR/CLIO-NRP-V7 complexes. CLIO-NRP-V7 appeared not to cause apparent cytotoxicity to the labeled cells, which demonstrated similar levels of cellular differentiation or secretion of cytokines such as interleukin-2 and IFN-γ. As a control, no uptake was found in NRP-V7–reactive CD8^+^ TCs that were incubated with CLIO-NH_2_ or CLIO conjugated with irrelevant peptides.

Medarova et al. examined the distribution of CLIO-NRP-V7–labeled CD8^+^ TCs in the pancreata of NOD mice with in vitro immunofluorescence microscopy and histological analysis (5). The excised pancreata were stained with an anti-CD3 monoclonal antibody and hematoxylin & eosin (H&E) staining. CLIO-NRP-V7–labeled CD8^+^ TCs were found in pancreatic islets and pancreatic lymph nodes as early as 5 weeks of age and reached a maximum at 8 weeks of age. The majority of CLIO-NRP-V7 was found to be localized in TCs. Light microscopy was also used to examine the excised pancreas stained with anti-CD8 (for CD8^+^ TCs) or anti-CD68 antibody (for macrophages). CLIO-NRP-V7 was found in both macrophages and CD8^+^ TCs. In comparison, NOD mice injected with CLIO-NH_2_ exhibited limited accumulation of the probe only in macrophages.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(CLIO-NRP-V7) +AND++rodentia)]

Moore et al. studied the in vivo binding of CLIO-NRP-V7 to autoreactive CD8^+^ TCs (1). 8.3-NOD mice or wild-type NOD mice were injected with CLIO-NRP-V7 (10 mg Fe/kg) intravenously, and blood was withdrawn 24 h later for FACS analysis. The labeling efficiency was ~90% for the peripheral blood CD8^+^ TCs derived from 8.3-NOD mice but ~2% for those derived from wild-type NOD mice. This result demonstrated that the systematic injection of CLIO-NRP-V7 allowed for selective in vivo labeling of NRP-V7–reactive CD8^+^ TCs. Moore et al. further tracked the homing of the labeled NRP-V7–reactive CD8^+^ TCs with in vivo MRI (1). NRP-V7–reactive CD8^+^ TCs derived from 8.3-NOD mice were labeled ex vivo with CLIO-NRP-V7 followed by intraperitoneal transferr into NOD SCID mice (5 weeks old, n = 5). MRI images were collected before and 1, 2, 4, 5, 9, and 13 days after cell transfer. The pancreata became darker over time in T_2_-weighted imaging, demonstrating the progressive accumulation of cells; no change in signal intensity was found in the spleen, liver, or muscle tissue. The change in signal intensity was noticeable from the second day after the cell transfer and continued up to day 16. The signal was diluted by in situ cellular proliferation of accumulated cells, but progressive recruitment and accumulation of labeled cells within the inflamed tissue compensated for this dilution. During this time, no alteration in blood glucose sugar was observed. To confirm the results, the animals were euthanized after MRI experiments, and pancreata were excised for histological staining and fluorescence microscopy analysis. H&E staining confirmed the infiltration of transferred lymphocytes in the islets. The fluorescence microscopy demonstrated the presence of FITC-positive CD8^+^ TCs in the pancreas.

Medarova et al. used CLIO-NRP-V7 to study the infiltration of CD8^+^ TCs in the pancreatic islets of NOD mice at different ages (5). CLIO-NRP-V7 (10 mg Fe/kg) was injected intravenously into female NOD mice at 5 (n = 7), 8 (n = 4), 15 (n = 4), and 24 (n = 10) weeks of age. T_2_-Weighted images were collected before and 24 h after injection with a 9.4-T imager. As a control, the same dose of CLIO-NH_2_ was injected to evaluate the contributions from nonspecific uptake of nanoparticles by macrophages. There was a significant change in pancreas for CLIO-NRP-V7 compared with that for CLIO-NH_2_, demonstrating antigen-specific accumulation of CLIO-NRP-V7. The signal decrease in pancreas reached its maximum in 8-week-old NOD mice. The animals were euthanized after the MRI experiments; their blood, splenocytes, and islets were isolated for flow cytometry analysis. The percentage of MION-NRP-V7–reactive CD8^+^ TCs in the blood peaked in 7- to 8-week-old mice but not in the spleen, indicating a high CLIO-NRP-V7–specific CD8^+^ TCs in the intra-islet lymphocyte population in the circulating pool. This result demonstrated a good correlation between the flow cytometry analysis and the MRI finding that the CD8+ intra-islet lymphocytes were highest in 8-week-old NOD mice.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(CLIO-NRP-V7) +AND+(primate+non+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(CLIO-NRP-V7) +AND+human)]

No publication is currently available.

### NIH Support

DK 64850, DK 63572

## References

1 Moore A., Grimm J., Han B., Santamaria P. (2004). Tracking the recruitment of diabetogenic CD8+ T-cells to the pancreas in real time. Diabetes.
2 Lieberman S.M., Evans A.M., Han B., Takaki T., Vinnitskaya Y., Caldwell J.A., Serreze D.V., Shabanowitz J., Hunt D.F., Nathenson S.G., Santamaria P., DiLorenzo T.P. (2003). Identification of the beta cell antigen targeted by a prevalent population of pathogenic CD8+ T cells in autoimmune diabetes. Proc Natl Acad Sci U S A.
3 Denis M.C., Mahmood U., Benoist C., Mathis D., Weissleder R. (2004). Imaging inflammation of the pancreatic islets in type 1 diabetes. Proc Natl Acad Sci U S A.
4 Brodie G.M., Wallberg M., Santamaria P., Wong F.S., Green E.A. (2008). B-cells promote intra-islet CD8+ cytotoxic T-cell survival to enhance type 1 diabetes. Diabetes.
5 Medarova Z., Tsai S., Evgenov N., Santamaria P., Moore A. (2008). In vivo imaging of a diabetogenic CD8+ T cell response during type 1 diabetes progression. Magn Reson Med.
6 Anderson B., Park B.J., Verdaguer J., Amrani A., Santamaria P. (1999). Prevalent CD8(+) T cell response against one peptide/MHC complex in autoimmune diabetes. Proc Natl Acad Sci U S A.
7 Josephson L., Perez J.M., Weissleder R. (2001). Magnetic nanosensors for the detection of oligonucleotide sequences. Angew. Chem. Int. Ed. Engl.
8 Bulte J.W., Brooks R.A., Moskowitz B.M., Bryant L.H., Frank J.A. (1998). T1 and T2 relaxometry of monocrystalline iron oxide nanoparticles (MION-46L): theory and experiment. Acad Radiol.
9 Mulder W.J., Strijkers G.J., Griffioen A.W., van Bloois L., Molema G., Storm G., Koning G.A., Nicolay K. (2004). A liposomal system for contrast-enhanced magnetic resonance imaging of molecular targets. Bioconjug Chem.
10 Wunderbaldinger P., Josephson L., Weissleder R. (2002). Crosslinked iron oxides (CLIO): a new platform for the development of targeted MR contrast agents. Acad Radiol.
11 Altman J.D., Moss P.A., Goulder P.J., Barouch D.H., McHeyzer-Williams M.G., Bell J.I., McMichael A.J., Davis M.M. (1996). Phenotypic analysis of antigen-specific T lymphocytes. Science.